# 5-(5-(2-(2-(2-[^18^F]Fluoroethoxy)ethoxy)ethoxy)benzofuran-2-yl)-N-methylbenzenamine

Chemical name: | 5-(5-(2-(2-(2-[^18^F]Fluoroethoxy)ethoxy)ethoxy)benzofuran-2-yl)-N-methylbenzenamine
Abbreviated name: | [^18^F]FPHBF-2
Synonym:
Agent category: | Compound
Target: | Amyloid-beta peptide
Target category: | Acceptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPHBF-2)]

Alzheimer's disease (AD) is a form of dementia with a gradual memory loss and a progressive decline in mental functions over time (1, 2). It is characterized pathologically by neuronal loss, extracellular senile plaques (aggregates of amyloid-β peptides consisting of 40–42 amino acids), and intracellular neurofibrillary tangles (filaments of microtubule-binding hyperphosphorylated protein tau) in the brain, especially in the hippocampus and associative regions of the cortex (3, 4). β-Amyloid peptides and tau proteins are implicated as the main causes of neuronal degeneration and cell death (5, 6).

Early diagnosis of AD is important for treatment consideration and disease management (7). Various β-amyloid imaging agents have been developed for magnetic resonance imaging (MRI), single-photon emission computed tomography, and positron emission tomography (PET) (8-13) as measures of the presence of plaque. The binding of different derivatives of Congo red, thioflavin, stibene, and aminonaphthalene has been studied in human post-mortem brain tissue and in transgenic mice. Of these analogs, 2-(1-(6-[(2-[^18^F]fluoroethyl)(methyl)amino]-2-naphthyl)ethylidene)malono nitrile ([^18^F]FDDNP) was studied in humans, and it showed more binding in the brains of patients with AD than in those of healthy people (14). However, [^18^F]FDDNP showed low signal/noise ratios for PET imaging because it is highly lipophilic. N-Methyl-[^11^C]-2-(4’-methylaminophenyl)-6-hydroxybenzothiasole, a β-amyloid binding compound based on a series of neutral thioflavin-T derivatives (15), was radiolabeled with the positron-emitting radionuclide ^11^C ([^11^C]6-OH-BTA-1 or [^11^C]PIB). [^11^C]6-OH-BTA-1 was found to be a promising imaging agent for senile plaques in the brain (10). 5-(5-(2-(2-(2-[^18^F]Fluoroethoxy)ethoxy)ethoxy)benzofuran-2-yl)-N,N-dimethylbenzenamine ([^18^F]FPHBF-1) was found to exhibit good initial uptake but slow washout from the brain in normal mice, and thus it is not suitable for imaging studies. Ono et al. (16) reported the development of the less lipophilic monomethylamino derivative of [^18^F]FPHBF-1, 5-(5-(2-(2-(2-[^18^F]fluoroethoxy)ethoxy)ethoxy)benzofuran-2-yl)-N-methylbenzenamine ([^18^F]FPHBF-2) as a PET imaging agent for β-amyloid plaques in the brain.

### Related Resource Links:

- Chapters in MICAD (Amyloid (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=amyloid+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (Amyloid (http://www.ncbi.nlm.nih.gov/gene/351))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Amyloid (http://www.ncbi.nlm.nih.gov/omim/?term=Amyloid))
- Clinical trials (Amyloid (http://www.clinicaltrials.gov/ct2/results?term=Amyloid))
- Drug information in FDA (Amyloid inhibitors (http://google2.fda.gov/search?q=Amyloid+inhibitor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=16&y=16))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPHBF-2%20and%20synthesis)]

[^18^F]FPHBF-2 was readily synthesized by standard ^18^F-fluorination of the N-BOC–protected mesylate derivative with [^18^F]KF/Kryptofix 2.2.2, for 5 min at 120°C and the subsequent acid hydrolysis with 10% HCl for 5 min at 120°C (16). [^18^F]FPHBF-2 was purified with high-performance liquid chromatography. Overall radiochemical yield was 52%, with a specific activity of 242 GBq/µmol (6.5 Ci/µmol) at the end of synthesis and a radiochemical purity of >99%. Total synthesis time was not reported. CLogP (lipophilicity) values were calculated to be 2.94 and 3.73 for [^18^F]FPHBF-2 and [^18^F]FPHBF-1, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPHBF-2%20and%20in%20vitro)]

FPHBF-2 has a binding affinity (K_i_) value of 3.85 ± 0.23 nM for aggregated β-amyloid(1–42) peptide in competition with [^125^I]IMPY (16). [^18^F]FPHBF-2 bound to the cortex of post-mortem AD brain slices but not to control brain slices as visualized with in vitro autoradiography studies.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPHBF-2%20and%20rodentia)]

[^18^F]FPHBF-2 (0.37 MBq (10 μCi)) was injected intravenously into normal male mice (n = 5/group) to study its accumulation in the brain and other organs/tissues at 2, 10, 30, and 60 min after injection (16). [^18^F]FPHBF-2 showed rapid penetration into the brain with 8.18 ± 0.59% injected dose (ID)/g at 2 min and a quick washout (3.87 ± 0.42% ID/g at 60 min). The brain_2min_/brain_60min_ value was 2.11. In comparison, [^18^F]FPHBF-1 exhibited a brain_2min_/brain_60min_ value of 1.02. The radioactivity levels at 60 min were 7.33% ID/g and 3.30% ID/g in the blood and bone, respectively. The bone radioactivity was 1.57% ID/g at 2 min. Ex vivo autoradiography studies of the brains of transgenic Tg2576 mice overexpressing β-amyloid plaques in the brain were performed after injection of [^18^F]FPHBF-2. The brains showed a distinctive labeling of β-amyloid plaques by co-staining with thioflavin-S. No such labeling and staining were observed in the control wild-type mice. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPHBF-2%20and%20%28dog%20or%20pig%20or%20cat%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPHBF-2%20and%20primate%20not%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPHBF-2%20and%20humans)]

No publication is currently available.

## References

1 Forstl H., Kurz A. (1999). Clinical features of Alzheimer's disease. Eur Arch Psychiatry Clin Neurosci.
2 Heininger K. (2000). A unifying hypothesis of Alzheimer's disease. IV. Causation and sequence of events. Rev Neurosci.
3 Mirra S.S., Heyman A., McKeel D., Sumi S.M., Crain B.J., Brownlee L.M., Vogel F.S., Hughes J.P., van Belle G., Berg L. (1991). The Consortium to Establish a Registry for Alzheimer's Disease (CERAD). Part II. Standardization of the neuropathologic assessment of Alzheimer's disease. Neurology.
4 Hardy J.A., Higgins G.A. (1992). Alzheimer's disease: the amyloid cascade hypothesis. Science.
5 Hardy J. (2003). The relationship between amyloid and tau. J Mol Neurosci.
6 Brandt R., Hundelt M., Shahani N. (2005). Tau alteration and neuronal degeneration in tauopathies: mechanisms and models. Biochim Biophys Acta.
7 de Leon M.J., DeSanti S., Zinkowski R., Mehta P.D., Pratico D., Segal S., Clark C., Kerkman D., DeBernardis J., Li J., Lair L., Reisberg B., Tsui W., Rusinek H. (2004). MRI and CSF studies in the early diagnosis of Alzheimer's disease. J Intern Med.
8 Bacskai B.J., Klunk W.E., Mathis C.A., Hyman B.T. (2002). Imaging amyloid-beta deposits in vivo. J Cereb Blood Flow Metab.
9 Nordberg A. (2004). PET imaging of amyloid in Alzheimer's disease. Lancet Neurol.
10 Klunk W.E., Engler H., Nordberg A., Wang Y., Blomqvist G., Holt D.P., Bergstrom M., Savitcheva I., Huang G.F., Estrada S., Ausen B., Debnath M.L., Barletta J., Price J.C., Sandell J., Lopresti B.J., Wall A., Koivisto P., Antoni G., Mathis C.A., Langstrom B. (2004). Imaging brain amyloid in Alzheimer's disease with Pittsburgh Compound-B. Ann Neurol.
11 Klunk W.E., Engler H., Nordberg A., Bacskai B.J., Wang Y., Price J.C., Bergstrom M., Hyman B.T., Langstrom B., Mathis C.A. (2003). Imaging the pathology of Alzheimer's disease: amyloid-imaging with positron emission tomography. Neuroimaging Clin N Am.
12 Wang Y., Klunk W.E., Debnath M.L., Huang G.F., Holt D.P., Shao L., Mathis C.A. (2004). Development of a PET/SPECT agent for amyloid imaging in Alzheimer's disease. J Mol Neurosci.
13 Kung M.P., Hou C., Zhuang Z.P., Skovronsky D., Kung H.F. (2004). Binding of two potential imaging agents targeting amyloid plaques in postmortem brain tissues of patients with Alzheimer's disease. Brain Res.
14 Shoghi-Jadid K., Small G.W., Agdeppa E.D., Kepe V., Ercoli L.M., Siddarth P., Read S., Satyamurthy N., Petric A., Huang S.C., Barrio J.R. (2002). Localization of neurofibrillary tangles and beta-amyloid plaques in the brains of living patients with Alzheimer disease. Am J Geriatr Psychiatry.
15 Bacskai B.J., Hickey G.A., Skoch J., Kajdasz S.T., Wang Y., Huang G.F., Mathis C.A., Klunk W.E., Hyman B.T. (2003). Four-dimensional multiphoton imaging of brain entry, amyloid binding, and clearance of an amyloid-beta ligand in transgenic mice. Proc Natl Acad Sci U S A.
16 Ono M., Cheng Y., Kimura H., Cui M., Kagawa S., Nishii R., Saji H. (2011). Novel (18)F-Labeled Benzofuran Derivatives with Improved Properties for Positron Emission Tomography (PET) Imaging of beta-Amyloid Plaques in Alzheimer's Brains. J Med Chem.